# 3-Cyano-4-[^18^F]fluoro-benzoyl-Arg-Ava-Gln-Trp-Ala-Val-NMeGly-His-Sta-Leu-NH_2_

Chemical name: | 3-Cyano-4-[^18^F]fluoro-benzoyl-Arg-Ava-Gln-Trp-Ala-Val-NMeGly-His-Sta-Leu-NH_2_ | [image]
Abbreviated name: | [^18^F]6b | [image]
Synonym: | | [image]
Agent Category: | Peptides | [image]
Target: | Gastrin-releasing peptide receptor (GRPR) | [image]
Target Category: | Receptors | [image]
Method of detection: | Positron emission tomography (PET) | [image]
Source of signal / contrast: | ^18^F | [image]
Activation: | No | [image]
Studies: | - In vitro; - Rodents | Structure of [^18^F]6b

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=GRPR+and+bombesin+and+imaging)]

3-Cyano-4-[^18^F]fluoro-benzoyl-Arg-Ava-Gln-Trp-Ala-Val-NMeGly-His-Sta-Leu-NH_2_, abbreviated as [^18^F]6b, is a bombesin (BN)-based ^18^F-labeled peptide synthesized by Mu et al. for positron emission tomography (PET) of tumors expressing gastrin-releasing peptide receptor (GRPR) (1).

BN is an amphibian neuropeptide consisting of 14 amino acids (pGlu-Gln-Arg-Leu-Gly-Asn-Gln-Trp-Ala-Val-Gly-His-Leu-Met-NH_2_) (2, 3). The C-terminal region of BN is responsible for its receptor binding and signal transduction. BN and its mammalian counterpart, gastrin-releasing peptide (GRP), produce a wide range of biological responses in diverse tissues (3). They also act as growth factors for cancer cells. Of the BN receptors, GRPR (also known as BB_2_ or BRS2) is best characterized (2). GRPR is a glycosylated G-protein–coupled receptor and is normally expressed in non-neuroendocrine tissues of the breast and pancreas and in neuroendocrine cells of the brain, gastrointestinal tract, lung, and prostate (3, 4). Because GRPR is overexpressed in various tumors, a large number of BN analogs have been tested for GRPR-targeted imaging and therapy (5, 6). These analogs have been synthesized on the basis of either truncated BN (6–14 or 7–14) or full-length BN (1–14), and most analogs exhibit a high affinity to GRPR (7, 8). The truncated BN analogs appear more stable in vivo than the full-length tetradecapeptides, but the full-length peptides offer more labeling options by attachment of functional groups to the amino acids on positions 1 to 6 (6, 9). For most analogs, the amino acids on positions 13 (Leu) and 14 (Met) have been replaced with non-natural amino acids for increasing stability, and Lys has been placed on position 3 for attaching radiolabels (1, 10). Spacers, chelators, or radiometals have also been widely used for conjugation and for favorable kinetics (1, 11, 12). Functionally, most BN analogs act as agonists, and only a few to date are antagonists (9). Agonists are internalized into and accumulate within cells, and they have been assumed to exhibit higher uptake by cancer cells than antagonists. However, some studies have shown that tumor uptake of antagonists is higher than that of agonists because antagonists may have stronger binding for GRPR than agonists (9).

Mu et al. synthesized a series of BN-based peptides by using different linkers, peptide sequences, and non-natural amino acids (1). These peptides have been labeled with ^18^F with a one-step approach via^18^F-for-^+^N(CH_3_)_3_ substitution using a less lipophilic benzonitrile labeling moiety. Amino acids such as His, Trp, Arg, and non-natural amino acids such as statine (Sta) and cysteine sulfonic acid (Ala(SO_3_H)) in the peptide sequence did not require any protection group during radiosynthesis. Two analogs, one named as [^18^F]6b and another [^18^F]7b, exhibited specific uptake in GRPR-expressing PC-3 tumors and the pancreas in nude mice (1). [^18^F]6b is positively charged, while [^18^F]7b is negatively charged. This chapter describes the data obtained with [^18^F]6b. The data obtained with [^18^F]7b are described in the MICAD chapter on [^18^F]7b (http://www.ncbi.nlm.nih.gov/books/NBK5330/).

### Related Resource Links:

- Protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&id=4885361), nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=nuccore&id=61677286) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?db=gene&cmd=Retrieve&dopt=full_report&list_uids=2925) information for GRPR
- Structure information of BN and analogs in PubChem (http://www.ncbi.nlm.nih.gov/pcsubstance/?term=bombesin)
- GRPR-targeted imaging agents in MICAD (http://www.ncbi.nlm.nih.gov/books/?term=GRPR%20AND%20micad%5bbook%5d)

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/20857927)]

Mu et al. synthesized [^18^F]6b on the basis of the amino acid sequence 7–14 of the natural BN (1). Met^14^ was replaced with Leu for stabilization against aminopeptidases, and Leu^13^ was replaced with Sta for prevention of neutral endopeptidase cleavage. Gly^11^ was changed to its methylated version (NMeGly). A polar spacer, Arg-Ava, was inserted between the labeling moiety and the binding sequence to improve the peptide pharmacokinetics and to avoid the interference of radiolabels with the binding region. The ^18^F labeling was carried out according to the method described by Becaud et al. (12). The reaction time was 15 min at 70°C. The ^18^F-incorporation was 51%. The decay-corrected radiochemical yield of [^18^F]6b was ~20%. The specific activity and radiochemical purity were not defined in this report (refer to Becaud et al. (12)). The lipophilicity, expressed as distribution coefficient D (log D_7.4_), was −1.1. The fluorinated peptide had calculated and found molecular weights of 1,381.7 and 692.4, respectively.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/20857927)]

The receptor binding affinity of [^18^F]6b was determined with the use of cell membranes transfected with human GRPR (1). Nonspecific binding was determined with an excess of 10 μM Tyr^4^-BN. The binding affinity of the non-labeled peptide (Arg-Ava-Gln-Trp-Ala-Val-NMeGly-His-Sta-Leu-NH_2_) was 0.7 nM, and its half maximal inhibitory concentration was 2.7 nM.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/20857927)]

The biodistribution of [^18^F]6b was studied in nude mice bearing subcutaneous PC-3 human prostate tumors (n = 3 mice/group) (1). The tumor uptake was 2.36 ± 0.47% injected dose per gram of tissue (ID/g) at 30 min after injection, which decreased slightly to 1.8 ± 1.56, 1.28 ± 0.27, and 1.61 ± 0.23% ID/g at 1, 2, and 4 h after injection, respectively. Similarly, uptake in the GRPR-rich pancreas reached 2.57 ± 0.03% ID/g at 30 min after injection and then decreased slightly over time. The binding of [^18^F]6b toward GRPR could be blocked by ~40% in the tumor and by ~60% in the pancreas at 60 min after injection, indicating that a large part of the tracer uptake in the tumor and pancreas can be attributed to specific GRPR binding. After the tumor and pancreas, the highest accumulation of [^18^F]6b was found in excretory organs, specifically the gallbladder, intestine, kidneys, and liver. Activity uptake in the gallbladder and intestine was much higher than uptake in the kidneys, suggesting a preponderance of hepatobiliary elimination versus renal excretion. The % ID/g values in bone were 4.36 ± 0.34, 4.64 ± 0.42, 7.80 ± 0.89, and 7.98 ± 1.58 at 0.5, 1, 2, and 4 h after injection, respectively. The increasing uptake in bone over time indicates that ^18^F-fluoride represents a major radiometabolite.

The comparative in vivo analysis of [^18^F]6b and [^18^F]7b showed that [^18^F]7b possesses superior characteristics with respect to the total tracer accumulation in tumors and the GRPR-rich pancreas and the specificity of uptake in target tissues (1). At physiological pH, Arg and Ala(SO_3_H) become positively and negatively charged, respectively. Although [^18^F]6b and [^18^F]7b bear the same binding peptide sequence and have the same lipophilicity, the charge of the linker obviously plays a major role in in vivo pharmacokinetics.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22%20SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

No references are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28primate%20NOT%20human%29)]

No references are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20human)]

No references are currently available.

## References

1 Mu L., Honer M., Becaud J., Martic M., Schubiger P.A., Ametamey S.M., Stellfeld T., Graham K., Borkowski S., Lehmann L., Dinkelborg L., Srinivasan A. (2010). In vitro and in vivo characterization of novel 18F-labeled bombesin analogues for targeting GRPR-positive tumors. Bioconjug Chem.
2 Ischia J., Patel O., Shulkes A., Baldwin G.S. (2009). Gastrin-releasing peptide: different forms, different functions. Biofactors.
3 Weber H.C. (2009). Regulation and signaling of human bombesin receptors and their biological effects. Curr Opin Endocrinol Diabetes Obes.
4 Smith C.J., Volkert W.A., Hoffman T.J. (2003). Gastrin releasing peptide (GRP) receptor targeted radiopharmaceuticals: a concise update. Nucl Med Biol.
5 Ananias H.J., de Jong I.J., Dierckx R.A., van de Wiele C., Helfrich W., Elsinga P.H. (2008). Nuclear imaging of prostate cancer with gastrin-releasing-peptide-receptor targeted radiopharmaceuticals. Curr Pharm Des.
6 Schroeder R.P., van Weerden W.M., Bangma C., Krenning E.P., de Jong M. (2009). Peptide receptor imaging of prostate cancer with radiolabelled bombesin analogues. Methods.
7 Smith C.J., Volkert W.A., Hoffman T.J. (2005). Radiolabeled peptide conjugates for targeting of the bombesin receptor superfamily subtypes. Nucl Med Biol.
8 Zhang X., Cai W., Cao F., Schreibmann E., Wu Y., Wu J.C., Xing L., Chen X. (2006). 18F-labeled bombesin analogs for targeting GRP receptor-expressing prostate cancer. J Nucl Med.
9 Cescato R., Maina T., Nock B., Nikolopoulou A., Charalambidis D., Piccand V., Reubi J.C. (2008). Bombesin receptor antagonists may be preferable to agonists for tumor targeting. J Nucl Med.
10 Nock B.A., Nikolopoulou A., Galanis A., Cordopatis P., Waser B., Reubi J.C., Maina T. (2005). Potent bombesin-like peptides for GRP-receptor targeting of tumors with 99mTc: a preclinical study. J Med Chem.
11 Hohne A., Mu L., Honer M., Schubiger P.A., Ametamey S.M., Graham K., Stellfeld T., Borkowski S., Berndorff D., Klar U., Voigtmann U., Cyr J.E., Friebe M., Dinkelborg L., Srinivasan A. (2008). Synthesis, 18F-labeling, and in vitro and in vivo studies of bombesin peptides modified with silicon-based building blocks. Bioconjug Chem.
12 Becaud J., Mu L., Karramkam M., Schubiger P.A., Ametamey S.M., Graham K., Stellfeld T., Lehmann L., Borkowski S., Berndorff D., Dinkelborg L., Srinivasan A., Smits R., Koksch B. (2009). Direct one-step 18F-labeling of peptides via nucleophilic aromatic substitution. Bioconjug Chem.